# 3'-(E)-(2-[^123/131^I]Iodovinyl)uridine

Chemical name: | 3'-(E)-(2-[^123/131^I]Iodovinyl)uridine
Abbreviated name: | [^123/131^I]IV-14
Synonym:
Agent category: | Compound
Target: | Uridine-cytidine kinase 2 (UCK2), human equilibrating nucleoside transporter 1 (hENT_1_)
Target category: | Enzyme, transporter
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal: | ^131^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IV-14)]

One of the characteristics of tumor cells is their unchecked proliferation. It is important to measure the proliferation rate of cancer lesions to help differentiate benign tumors from malignant tumors and to characterize malignant tumors among normal tissues. 2-[^18^F]Fluoro-2-deoxy-D-glucose ([^18^F]FDG) has been approved (http://www.fda.gov/Drugs/DevelopmentApprovalProcess/Manufacturing/ucm182642.htm) for cancer imaging by the United States Food and Drug Administration. However, enhanced uptake of FDG also occurs in inflammatory cells and lesions as well as in necrotic cells (1, 2). Thymidine (TdR) and TdR analogs are the standard markers for DNA synthesis, and [^11^C]TdR has been used in positron emission tomography (PET) imaging to measure tumor growth rate in situ. Because of the short half-life of ^11^C and the extensive metabolism of [^11^C]TdR in the blood (3), 3'-deoxy-3'-[^18^F]fluorothymidine (FLT) was developed for PET imaging. FLT is an analog of TdR and is phosphorylated by TdR kinase-1 (TK-1), an enzyme expressed during the DNA synthesis phase (S-phase) of the cell cycle (4). On the other hand, RNA synthesis occurs in all phases of the cell cycle except the M phase, even in slow growing solid tumors. Tracers targeted to RNA synthesis could be used to visualize tumors with low TK-1 expression.

Phosphorylation of pyrimidine ribonucleosides is carried out with uridine-cytidine kinase (UCK) 1 and UCK2 (5). UCK2 is normally present only in human placenta (5) and testis (6) but is highly overexpressed in many blood and solid tumor cells (7). UCK1 is ubiquitously expressed in normal tissues. Phosphorylation of uridine and cytosine is 15–20 times faster with UCK2 than with UCK1. 3'-(Ethynyl)uridine is phosphorylated rapidly with UCK2 to its triphosphate, which blocks RNA synthesis by inhibition of RNA polymerase (8, 9). Zlatopolskiy et al. (10) reported the development of 3'-(E)-(2-[^123/131^I]iodovinyl)uridine ([^123/131^I]IV-14) for single-photon emission computed tomography (SPECT) imaging of UCK2 activity in tumors.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Uridine-cytidine%20kinase%20+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (UCK2, (http://www.ncbi.nlm.nih.gov/gene/7371) human equilibrating nucleoside transporter 1 (http://www.ncbi.nlm.nih.gov/gene/2030)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=609329)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=131I-IV-14%20and%20synthesis)]

Zlatopolskiy et al. (10) reported the synthesis of [^123/131^I]IV-14 by the standard chloramine-T radioiodination of 3'-(2-E)-tributylstannylvinyl-uridine (4.4 ng) in the presence of ^123/131^I-NaI (159 MBq (4.3 mCi)). [^123/131^I]IV-14 was purified with high-performance liquid chromatography with a radiochemical purity of >99% and a radiochemical yield of 71–82% (n = 12). The specific activity of [^123/131^I]IV-14 was not reported. [^131^I]IV-14 was stable in human serum for 24 h at 37ºC, whereas [^131^I]iododeoxyuridine was only 30% intact.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=131I-IV-14%20and%20in%20vitro)]

In vitro enzyme assays of uridine phosphorylase with murine liver, mucosa, or intestine homogenates revealed that [^131^I]IV-14 was resistant to hydrolysis of the uridine-to-glycosidic bond (10). In vitro cellular uptake assays with various cell lines showed that MIA PaCa-2, Panc-1, and CX-1 had high to moderate UCK2 and human equilibrating nucleoside transporter 1 (hENT_1_) expression with high uptake of [^131^I]IV-14 (2.24–4.27% incubation dose at 24 h after incubation). On the other hand, uptake of [^131^I]IV-14 was marginal with BX-PC-3 and SK-PC-1cell lines (<0.5%), which had low expression of UCK2 and hENT_1_. Interestingly, high accumulation (2.69%) of radioactivity was observed in HL60 cells with low UCK2 but high hENT_1_ expression. The uptake was inhibited by a highly selective inhibitor of hENT_1_ in HL60 and MIA PaCa-2 cells by 83% and 40% at 24 h of incubation, respectively. More than 90% of radioactivity was detected in the cytosolic fraction of HL60 cells with <5% in the RNA fraction. Mono-, di-, and tri-phosphate metabolites of [^131^I]IV-14 were found at various time points in HL60 cells pretreated with 5-fluorouridine.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=131I-IV-14%20and%20rodentia)]

Zlatopolskiy et al. (10) performed ex vivo biodistribution studies after injection of 10 MBq (270 μCi) [^123^I]IV-14 in nude mice (n = 5/group) bearing HL60 tumors. There was high tumor radioactivity uptake, low normal organ radioactivity uptake, and rapid body clearance. The tumor radioactivity levels after injection were 1.4% injected dose per gram (% ID/g) at 0.5 h, 1.5% ID/g at 1 h, 0.5% ID/g at 4 h, and 0.1% ID/g at 24 h. At 0.5 h, the radioactivity levels in other major organs (spleen, intestine, liver, stomach, and kidneys) were slightly higher than in the tumor but decreased progressively with time except in the tumor and spleen. At 0.5 h, the tumor/tissue ratios were 0.37, 0.68, 0.68, 0.72, and 1.05 for the kidneys, small intestine, liver, spleen, and blood, respectively. At 4 h, the tumor/tissue ratios were 10, 7, 16, 3, and 30 for the kidneys, small intestine, liver, spleen, and blood, respectively. Gamma planar imaging was performed in nude mice bearing HL60 tumors. Good visualization was observed only in the tumor, stomach, and spleen at 4 h after injection. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=131I-IV-14%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=131I-IV-14%20and%20(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=131I-IV-14%20and%20human)]

No publication is currently available.

## References

1 Kubota R., Yamada S., Kubota K., Ishiwata K., Tamahashi N., Ido T. (1992). Intratumoral distribution of fluorine-18-fluorodeoxyglucose in vivo: high accumulation in macrophages and granulation tissues studied by microautoradiography. J Nucl Med.
2 van Waarde A., Cobben D.C., Suurmeijer A.J., Maas B., Vaalburg W., de Vries E.F., Jager P.L., Hoekstra H.J., Elsinga P.H. (2004). Selectivity of 18F-FLT and 18F-FDG for differentiating tumor from inflammation in a rodent model. J Nucl Med.
3 Ishiwata K., Ido T., Abe Y., Matsuzawa T., Murakami M. (1985). Studies on 18F-labeled pyrimidines III. Biochemical investigation of 18F-labeled pyrimidines and comparison with 3H-deoxythymidine in tumor-bearing rats and mice. Eur J Nucl Med.
4 Sherley J.L., Kelly T.J. (1988). Regulation of human thymidine kinase during the cell cycle. J Biol Chem.
5 Van Rompay A.R., Norda A., Linden K., Johansson M., Karlsson A. (2001). Phosphorylation of uridine and cytidine nucleoside analogs by two human uridine-cytidine kinases. Mol Pharmacol.
6 Ozaki K., Kuroki T., Hayashi S., Nakamura Y. (1996). Isolation of three testis-specific genes (TSA303, TSA806, TSA903) by a differential mRNA display method. Genomics.
7 Murata D., Endo Y., Obata T., Sakamoto K., Syouji Y., Kadohira M., Matsuda A., Sasaki T. (2004). A crucial role of uridine/cytidine kinase 2 in antitumor activity of 3'-ethynyl nucleosides. Drug Metab Dispos.
8 Yokogawa T., Naito T., Kanda H., Takatori S., Takenaka K., Sasaki T., Matsuda A., Fukushima M., Kim H.S., Wataya Y. (2005). Inhibitory mechanisms of 1-(3-C-ethynyl-beta-D-ribopentofuranosyl)uracil (EUrd) on RNA synthesis. Nucleosides Nucleotides Nucleic Acids.
9 Takatori S., Kanda H., Takenaka K., Wataya Y., Matsuda A., Fukushima M., Shimamoto Y., Tanaka M., Sasaki T. (1999). Antitumor mechanisms and metabolism of the novel antitumor nucleoside analogues, 1-(3-C-ethynyl-beta-D-ribo-pentofuranosyl)cytosine and 1-(3-C-ethynyl-beta-D-ribo-pentofuranosyl)uracil. Cancer Chemother Pharmacol.
10 Zlatopolskiy B.D., Morgenroth A., Kunkel F.H., Urusova E.A., Dinger C., Kull T., Lepping C., Reske S.N. (2009). Synthesis and biologic study of IV-14, a new ribonucleoside radiotracer for tumor visualization. J Nucl Med.